# ^111^In-Labeled diethylenetriamine-pentaacetic acid-Ac-TZ14011

Chemical name: | ^111^In-Labeled diethylenetriamine pentaacetic acid-Ac-TZ14011 | [image]
Abbreviated name: | [^111^In]Ac-TZ14011 | [image]
Synonym: | [^111^In]-DTPA-Ac-TZ14011 | [image]
Agent Category: | Ligand | [image]
Target: | Chemokine receptor 4 (CXCR4) | [image]
Target Category: | Receptor | [image]
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging | [image]
Source of signal / contrast: | ^111^In | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of ^111^In-DTPA-Ac-TZ14011 (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ac+TZ14011)]

The chemokine receptor 4 (CXCR4) and its ligand, the stromal cell–derived factor-1 (SDF-1 or CXCL12), are known to play a major role in the migration of progenitor cells during embryonic development of the central nervous, cardiovascular, and the hematopoietic systems (2, 3). In addition, this receptor–ligand pair has a function in the development, progression, and spread of various cancers (4), and the CXCR4 acts as a co-receptor to facilitate entry of the human immunodeficiency virus (HIV) into CD4^+^ cells (5). It has also been suggested that CXCR4 and SDF-1 participate in the pathogenesis of neurodegenerative and inflammatory conditions (6). The level of CXCR4 expression by tumor cells is considered to play a critical role in cancer metastasis by generation of a chemotactic gradient to organs expressing the SDF-1, and the overexpression of CXCR4 indicates a poor prognosis for patients suffering from different types of cancer (7). The role of CXCR4 (http://clinicaltrials.gov/ct2/results?term=CXCR4) and SDF-1 (http://clinicaltrials.gov/ct2/results?term=SDF-1) for cancer metastasis is under investigation in several clinical trials approved by the United States Food and Drug Administration.

Because CXCR4 and SDF-1 are considered to have a critical role in the development and progression of HIV infections and cancer, some imaging studies have been performed to quantify CXCR4 levels under in vivo conditions for various pathological and physiological conditions (8). Technetium (^99m^Tc)-labeled SDF-1 was used as a probe to determine changes in CXCR4 expression in the heart after a myocardial infarction, and it was concluded that [^99m^Tc]-SDF-1was a suitable probe to visualize CXCR4 expression in tissue with single-photon emission computed tomography (SPECT). In another study, copper (^64^Cu)-labeled 1,1’-{1,4-phenylenebis(methylene)}-bis{1,4,8,11-tetraaza-cyclotetradecane} (AMD3100), an inhibitor of CXCR4 activity, was used to perform imaging, and biodistribution of the radiochemical in normal mice was studied with positron emission tomography (9). This study showed that [^64^Cu]-AMD3100 accumulated mainly in the liver, kidneys, and spleen of the animals. An indium (^111^In)-labeled CXCR4 antagonist peptide, [^111^In]-Ac-TZ14011, discussed in this chapter, was developed for the imaging of CXCR4 expression in xenograft tumors in mice; Hanaoka et al. used SPECT to investigate the biodistribution of [^111^In]-Ac-TZ14011 in the animals (1).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ac+TZ14011+synthesis)]

The Ac-TZ14011 peptide was synthesized using Fmoc-based solid-phase synthesis and purified as described by Hanaoka et al. (1). The purified peptide was then conjugated with mono-reactive (or monoanhydride) diethylenetriamine-pentaacetic acid and purified to obtain DTPA-Ac-TZ14011 as detailed elsewhere (1).

For the labeling with ^111^In, DTPA-Ac-TZ14011 in 0.1 M acetic acid was mixed with (^111^In) indium chloride, and the mixture was left at room temperature for 30 min (1). The labeled product [^111^In]-DTPA-Ac-TZ14011 was purified with reverse-phase high-performance liquid chromatography (RP-HPLC), and its purity was determined with thin-layer chromatography, cellulose acetate electrophoresis, and RP-HPLC. The radiochemical purity of [^111^In]-DTPA-Ac-TZ14011 was reported to be >96% as determined with the various analytical techniques mentioned above. The radiochemical yield of the synthesis and specific activity and stability of the radiochemical were not reported.

Using the same procedure detailed above, unlabeled In-DTPA-Ac-TZ14011 was also synthesized for use in some studies (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ac+TZ14011+in+vitro)]

Binding assays were performed using Chinese hamster ovary cells stably transfected with CXCR4 as described by Hanaoka et al. (1). Using different concentrations of ^131^I labeled stromal cell-derived factor 1α (a natural ligand of CXCR4) as a probe the 50% inhibitory concentrations of Ac-TZ14011 and In-DTPA-Ac-TZ14011 were determined to be 1.2 and 7.9 nM, respectively, under these experimental conditions.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ac+TZ14011+rodentia)]

Hanaoka et al. investigated the biodistribution of [^111^In]-DTPA-Ac-TZ14011 in nude mice bearing CXCR4-expressing pancreatic carcinoma AsPc-1 cell tumors (1). The radiochemical was administered intravenously to the animals, and the mice were euthanized at 1, 6, and 24 h (n = 5 mice/time point). For competition studies, another group of animals (n = 5 mice) were treated with [^111^In]-DTPA-Ac-TZ14011 in the presence of unlabeled Ac-TZ14011 (10 mg/kg body weight) and euthanized 1 h later. The major organs and the tumors were removed from all animals of the respective groups, and the amount of accumulated radioactivity (expressed as % of injected dose/gram tissue (% ID/g)) was determined. In animals treated with the radiochemical alone, a rapid clearance of radioactivity from the blood was reported, and during the same period an accumulation of the label was observed in the liver, kidneys, and the spleen (27.0 ± 2.9, 50.9 ± 4.3, and 8.22 ± 0.70% ID/g, respectively) at 1 h after treatment. Compared to the blood (0.39 ± 0.06 ID%/g) and muscles (0.17 ± 0.05%ID/g) a higher accumulation of radioactivity was observed in the tumors (0.51 ± 0.08%ID/g) at 1 h after treatment with the label. During the same time, animals in the competition study showed a significantly (P < 0.005) reduced accumulation of radioactivity only in the liver and the spleen (1.95 ± 0.25 and 2.66 ± 1.12% ID/g, respectively), and an insignificant change in accumulation of the label in the kidneys (45.4 ± 6.8% ID/g) was reported. The tumor/blood ratio of the radioactivity increased from 1.31 ± 0.14 to 5.65 ± 2.59 from 1 to 24 h after the treatment. For the competition animals, the ratio was 0.88 ± 0.31 at 1 h after injection of the radiochemical (significant at P < 0.05). The tumor/muscle ratio (T/M ratio) remained almost unchanged from 1 to 24 h (3.17 ± 0.99 and 3.23 ± 1.08, respectively), and the animals treated with the labeled compound in presence of the unlabeled molecule had a significantly (P < 0.005) reduced accumulation of radioactivity at 1 h after administration of the radiochemical (T/M ratio was 1.31 ± 0.41).

From these studies the investigators concluded that although [^111^In]-DTPA-Ac-TZ14011 could be used as an imaging agent for tumors overexpressing CXCR4 receptors, it was not suitable to detect such tumors in the liver, kidneys, and spleen because these organs accumulated a high amount of radioactivity after treatment with this radiotracer.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ac+TZ14011+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ac+TZ14011+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ac+TZ14011+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimer]

No information is currently available.

## References

1 Hanaoka H., Mukai T., Tamamura H., Mori T., Ishino S., Ogawa K., Iida Y., Doi R., Fujii N., Saji H. (2006). Development of a 111In-labeled peptide derivative targeting a chemokine receptor, CXCR4, for imaging tumors. Nucl Med Biol.
2 Juarez J., Bendall L. (2004). SDF-1 and CXCR4 in normal and malignant hematopoiesis. Histol Histopathol.
3 Miller R.J., Banisadr G., Bhattacharyya B.J. (2008). CXCR4 signaling in the regulation of stem cell migration and development. J Neuroimmunol.
4 Rubin J.B. (2009). Chemokine signaling in cancer: one hump or two?. Semin Cancer Biol.
5 Alkhatib G. (2009). The biology of CCR5 and CXCR4. Curr Opin HIV AIDS.
6 Mocchetti I., Bachis A., Masliah E. (2008). Chemokine receptors and neurotrophic factors: potential therapy against aids dementia?. J Neurosci Res.
7 Gelmini S., Mangoni M., Serio M., Romagnani P., Lazzeri E. (2008). The critical role of SDF-1/CXCR4 axis in cancer and cancer stem cells metastasis. J Endocrinol Invest.
8 Misra P., Lebeche D., Ly H., Schwarzkopf M., Diaz G., Hajjar R.J., Schecter A.D., Frangioni J.V. (2008). Quantitation of CXCR4 expression in myocardial infarction using 99mTc-labeled SDF-1alpha. J Nucl Med.
9 Jacobson O., Weiss I.D., Szajek L., Farber J.M., Kiesewetter D.O. (2009). 64Cu-AMD3100--a novel imaging agent for targeting chemokine receptor CXCR4. Bioorg Med Chem.